# [^11^C]Carfentanil

Chemical name: | [^11^C]Carfentanil
Abbreviated name: | [^11^C]CFN, [^11^C]CAR
Synonym:
Agent category: | Compound
Target: | Mu (μ) opioid receptor
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20carfentanil)]

Opioids such as morphine are commonly used analgesics in clinical practice. Three opioid receptors (mu, µ; delta, δ; and kappa, κ) that mediate opioid effects have been identified by molecular cloning: δ (enkephalin-preferring), κ (dynorphin-preferring), and µ (morphine and ß-endorphin-preferring) (1). Each type of opioid receptor consists of subtypes of receptors as suggested by pharmacological studies (2, 3). Their specificity and ubiquitous location are present in both the central and peripheral nervous system. The opioid receptors (G-protein coupled, resulting in decrease in adenylyl cyclase activity) play an important role in the regulation of analgesia, shock, appetite, thermoregulation, cardiovascular, mental and endocrine function (2-5). Although µ opioid receptors are the major receptor to mediate the analgesic effects of opioids, δ and κ receptors are also important in antinociception. Opioids have been found to protect cells from ischemia injury in the heart and brain via the δ receptors. On the other hand, κ antagonist prevents neurodegeneration.

The µ opioid receptors are localized predominately in the hypothalamus and thalamus, and the δ opioid receptors are localized predominately in the striatum, limbic system, and cerebral cortex (6, 7). The κ opioid receptors (κ_1_ and κ_2_ ) are the most abundant brain opioid receptors and are widely distributed in deeper layers of the neocortex (temporal, parietal, and frontal cortices), striatum, amygdala, and thalamus, with lower levels in the hippocampus, occipital cortex, and cerebellum (8-10). The µ opioid receptors have been implicated in several clinical brain disorders, including drug and alcohol abuses, epilepsy, and pain pathways (11-14).

Diprenorphine is a highly potent and nonselective opioid receptor antagonist with subnanomolar affinity (7). Diprenorphine was labeled as [6-O-methyl-^11^C]diprenorphine ([^11^C]DPN (http://www.ncbi.nlm.nih.gov/books/NBK23399/)) (15, 16). [^11^C]DPN has been employed as a positron emission tomography (PET) agent for the non-invasive studies of opioid receptors in the brain of patients with pain, Huntington's disease, Parkinson’s disease, and epilepsy. Carfentanil (CFN) is a highly potent and selective µ opioid receptor agonist with subnanomolar affinity (K_i_, 0.024 nM) (17). [^11^C]CFN is being developed as a PET agent for the non-invasive study of µ opioid receptors in the brain.

### Related Resource Links:

- Chapters in MICAD (opioid receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=opioid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (µ opioid receptor (http://www.ncbi.nlm.nih.gov/gene/4988), δ opioid receptor (http://www.ncbi.nlm.nih.gov/gene/4985))
- Articles in Online Mendelian Inheritance in Man (OMIM) (µ opioid receptor (http://www.ncbi.nlm.nih.gov/omim/600018), δ opioid receptor (http://www.ncbi.nlm.nih.gov/omim/165195))
- Clinical trials (opioid receptors (http://www.clinicaltrials.gov/ct2/results?term=opioid+receptors+))
- Drug information in FDA (opioid receptors (http://google2.fda.gov/search?q=opioid+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20carfentanil%20and%20synthesis)]

Dannals et al. (18) reported synthesis of [^11^C]CFN by [^11^C]-O-methylation of the carboxylate precursor as sodium salt with [^11^C]methyl iodide. An average radiochemical yield was ~30% based on [^11^C]CO_2_ after HPLC purification with a total synthesis time of 30 min. An average specific activity was 42.6 GBq/μmol (1.15 Ci/μmol at end of synthesis) with a radiochemical purity of >97%.

Jewett et al. (19) reported a modified procedure for synthesis of [^11^C]CFN using an extraction disk instead of high-performance liquid chromatography (HPLC). The carboxylate precursor as the tetrabutylammonium salt was reacted at room temperature for 5 min with [^11^C]methyl triflate. [^11^C]CFN was trapped on a high performance extraction disk, and starting materials were selectively washed off. [^11^C]CFN was eluted with a small volume of ethanol. Radioactive contaminants were further removed by a small column of fibrous anion exchanger. The total synthesis time was ~10 min after purification. [^11^C]CFN was obtained in an averaged 15.6% radiochemical yield based on [^11^C]CO_2_ with a specific activity of 129.5 GBq/μmol (3.5 Ci/μmol) at end of synthesis. The radiochemical purity was >97%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20carfentanil%20and%20in%20vitro)]

Titeler et al. (20) reported that [^3^H]CFN had a K_d_ of 0.08 ± 0.01 nM and a B_max_ of 84 ± 3 fmol/mg tissue in vitro binding assays using human thalamic membranes. Cometta-Morini et al. (17) reported that CFN had K_i_ values of 0.024, 3.28, and 43.1 nM for the µ, δ, and κ opioid receptors, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20carfentanil%20and%20rodentia)]

Saji et al. (21) demonstrated a high accumulation of [^11^C]CFN in the mouse brain with 3.73% injected dose/g (ID/g) at 5 min, 2.85%ID/g at 15 min, 2.13%ID/g at 30 min, and 1.28%ID/g at 60 min after injection (n = 4). The highest accumulation was in the thalamus, followed by the striatum, cortex, and cerebellum at all time points studied. Coinjection of [^11^C]CFN with naloxone (1 mg/kg) inhibited the accumulation by 73-74% in the thalamus and 62-82% in the striatum, whereas only marginal inhibition was observed in the cortex and cerebellum. Jewett et al. (22) reported that the hypothalamus exhibited a higher accumulation than the thalamus in the rats and mice. Regional binding potentials (BPs) were determined in the rat brain using bolus infusion of 96-178 MBq (2.6-4.8 mCi) of [^11^C]CFN with the cerebellum as the reference tissue (n = 4). The BP values were 4.81 ± 0.59, 3.30 ± 0.78, 3.06 ± 0.20, 2.21 ± 0.31, 1.97 ± 0.19, and 1.49 ± 0.26 for the hypothalamus, striatum, thalamus, cortex, hippocampus, and pons/medulla, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20carfentanil%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20carfentanil%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20carfentanil%20and%20human)]

Frost et al. (23, 24) reported [^11^C]CFN PET studies in human brain using reference methods or kinetic modeling. High concentrations of radioactivity were observed in the basal ganglia and thalamus, intermediate concentrations in the frontal and parietal cerebral cortex, and low concentrations in the cerebellum and occipital cortex. Naloxone pretreatment (1 mg/kg) inhibited ~90% of [^11^C]CFN binding in the caudate nucleus (K_3_/K_4_, from 3.4 to 0.26) and medial thalamus (K_3_/K_4_, from 1.8 to 0.16) for the period 30-60 min after tracer injection. Endres et al. (25) performed [^11^C]CFN PET studies with arterial blood sampling in six healthy male control subjects. Specific binding estimates obtained from reference-tissue methods were compared to those obtained with a more rigorous blood input modeling technique. It was determined that both a graphical method and a simplified reference tissue model were more accurate than the tissue-ratio method for quantification of [^11^C]CFN binding. The regional binding potentials obtained with all methods showed excellent correlation (r >0.97) with each other.

Mayberg et al. (26) reported that [^11^C]CFN binding (µ opioid receptors) in eleven patients with idiopathic epilepsy was increased in the temporal neocortex and decreased in the amygdala on the side of the epileptic focus. [^11^C]DPN binding (all opioid subtypes) was not significantly different among regions in the focus and nonfocus temporal lobes.

Newberg et al. (27) estimated the human dosimetry of [^11^C]CFN in 5 healthy subjects after injection of 280 MBq (7.6 mCi) of [^11^C]CFN. The organ receiving the highest radiation dose was the urinary bladder at 0.0365 mGy/MBq(0.135 rad/mCi). The effective dose was 4.6 μSv/MBq.

[^11^C]CFN has allowed studies of μ opioid receptors in patients with epilepsy, pains, lung carcinoma as well as drug, smoking and alcohol addictions [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20carfentanil%20and%20human)].

## References

1 Minami M., Satoh M. (1995). Molecular biology of the opioid receptors: structures, functions and distributions. Neurosci Res.
2 Waldhoer M., Bartlett S.E., Whistler J.L. (2004). Opioid receptors. Annu Rev Biochem.
3 Satoh M., Minami M. (1995). Molecular pharmacology of the opioid receptors. Pharmacol Ther.
4 Molina P.E. (2006). Opioids and opiates: analgesia with cardiovascular, haemodynamic and immune implications in critical illness. J Intern Med.
5 Barry U., Zuo Z. (2005). Opioids: old drugs for potential new applications. Curr Pharm Des.
6 Chang K.J., Cooper B.R., Hazum E., Cuatrecasas P. (1979). Multiple opiate receptors: different regional distribution in the brain and differential binding of opiates and opioid peptides. Mol Pharmacol.
7 Pfeiffer A., Pasi A., Mehraein P., Herz A. (1982). Opiate receptor binding sites in human brain. Brain Res.
8 Hiller J.M., Fan L.Q. (1996). Laminar distribution of the multiple opioid receptors in the human cerebral cortex. Neurochem Res.
9 Peckys D., Landwehrmeyer G.B. (1999). Expression of mu, kappa, and delta opioid receptor messenger RNA in the human CNS: a 33P in situ hybridization study. Neuroscience.
10 Simonin F., Gaveriaux-Ruff C., Befort K., Matthes H., Lannes B., Micheletti G., Mattei M.G., Charron G., Bloch B., Kieffer B. (1995). kappa-Opioid receptor in humans: cDNA and genomic cloning, chromosomal assignment, functional expression, pharmacology, and expression pattern in the central nervous system. Proc Natl Acad Sci U S A.
11 Lever J.R. (2007). PET and SPECT imaging of the opioid system: receptors, radioligands and avenues for drug discovery and development. Curr Pharm Des.
12 Ravert H.T., Bencherif B., Madar I., Frost J.J. (2004). PET imaging of opioid receptors in pain: progress and new directions. Curr Pharm Des.
13 Sprenger T., Berthele A., Platzer S., Boecker H., Tolle T.R. (2005). What to learn from in vivo opioidergic brain imaging?. Eur J Pain.
14 Ravert H.T., Mathews W.B., Musachio J.L., Scheffel U., Finley P., Dannals R.F. (1999). [11C]-methyl 4-[(3,4-dichlorophenyl)acetyl]-3-[(1-pyrrolidinyl)-methyl]-1- piperazinecarboxylate ([11C]GR89696): synthesis and in vivo binding to kappa opiate receptors. Nucl Med Biol.
15 Lever J.R., Dannals R.F., Wilson A.A., Ravert H.T., Wagner H.N. (1987). Synthesis of carbon-11 labeled diprenorphine: a radioligand for positron emission tomographic studies of opiate receptors. Tetrahedron Letters.
16 Luthra S.K., Brady F., Turton D.R., Brown D.J., Dowsett K., Waters S.L., Jones A.K., Mathews R.W., Crowder J.C. (1994). Automated radiosyntheses of [6-O-methyl-11C]diprenorphine and [6-O-methyl-11C]buprenorphine from 3-O-trityl protected precursors. Appl Radiat Isot.
17 Cometta-Morini C., Maguire P.A., Loew G.H. (1992). Molecular determinants of mu receptor recognition for the fentanyl class of compounds. Mol Pharmacol.
18 Dannals R.F., Ravert H.T., Frost J.J., Wilson A.A., Burns H.D., Wagner H.N. (1985). Radiosynthesis of an opiate receptor binding radiotracer: [11C]carfentanil. Int J Appl Radiat Isot.
19 Jewett D.M. (2001). A simple synthesis of [11C]carfentanil using an extraction disk instead of HPLC. Nucl Med Biol.
20 Titeler M., Lyon R.A., Kuhar M.J., Frost J.F., Dannals R.F., Leonhardt S., Bullock A., Rydelek L.T., Price D.L., Struble R.G. (1989). Mu opiate receptors are selectively labelled by [3H]carfentanil in human and rat brain. Eur J Pharmacol.
21 Saji H., Tsutsumi D., Magata Y., Iida Y., Konishi J., Yokoyama A. (1992). Preparation and biodistribution in mice of [11C]carfentanil: a radiopharmaceutical for studying brain mu-opioid receptors by positron emission tomography. Ann Nucl Med.
22 Jewett D.M., Kilbourn M.R. (2004). In vivo evaluation of new carfentanil-based radioligands for the mu opiate receptor. Nucl Med Biol.
23 Frost J.J., Douglass K.H., Mayberg H.S., Dannals R.F., Links J.M., Wilson A.A., Ravert H.T., Crozier W.C., Wagner H.N. (1989). Multicompartmental analysis of [11C]-carfentanil binding to opiate receptors in humans measured by positron emission tomography. J Cereb Blood Flow Metab.
24 Frost J.J., Wagner H.N., Dannals R.F., Ravert H.T., Links J.M., Wilson A.A., Burns H.D., Wong D.F., McPherson R.W., Rosenbaum A.E., et al. (1985). Imaging opiate receptors in the human brain by positron tomography. J Comput Assist Tomogr.
25 Endres C.J., Bencherif B., Hilton J., Madar I., Frost J.J. (2003). Quantification of brain mu-opioid receptors with [11C]carfentanil: reference-tissue methods. Nucl Med Biol.
26 Mayberg H.S., Sadzot B., Meltzer C.C., Fisher R.S., Lesser R.P., Dannals R.F., Lever J.R., Wilson A.A., Ravert H.T., Wagner H.N., et al. (1991). Quantification of mu and non-mu opiate receptors in temporal lobe epilepsy using positron emission tomography. Ann Neurol.
27 Newberg A.B., Ray R., Scheuermann J., Wintering N., Saffer J., Schmitz A., Freifelder R., Karp J., Lerman C., Divgi C. (2009). Dosimetry of 11C-carfentanil, a micro-opioid receptor imaging agent. Nucl Med Commun.